# Cypate-2-Deoxy-D-glucose

Chemical name: | Cypate-2-Deoxy-D-glucose
Abbreviated name: | Cypate-2DG
Synonym:
Agent category: | Compound
Target: | Glucose transporters, hexokinases
Target category: | Transporter, enzyme
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | Cypate
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cypate-2DG)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–650 nm) are used. Near-infrared (NIR) fluorescence (650–900 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a noninvasive complement to radionuclide imaging in small animals or with probes in close proximity to the target in humans (4). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (5-8). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon.

The phosphorylation of glucose, an initial and important step in cellular metabolism, is catalyzed by hexokinases (HKs) (9). There are four HKs in mammalian tissues (HKI–HKIV). HKI, HKII, and HKIII have molecular weights of ~100,000 each; HKI is found mainly in the brain, and HKII is insulin-sensitive and is found in adipose and muscle cells. HKIV, also known as glucokinase, has a molecular weight of ~50,000 and is specific to the liver and pancreas. Most brain HK is bound to mitochondria, enabling coordination between glucose consumption and oxidation. Tumor cells are known to be highly glycolytic because of increased expression of glycolytic enzymes and HK activity (10), which was detected in tumors from patients with lung, gastrointestinal, and breast cancers. The HKs, by converting glucose to glucose-6-phosphate, help maintain the downhill gradient that results in the transport of glucose into cells through the facilitative glucose transporters (GLUT1–13) (11). GLUT1 is considered to be the main transporter of glucose uptake. GLUT4 and HKII are the major transporter and HK isoform in skeletal muscle, heart, and adipose tissue, wherein insulin promotes glucose utilization. HKIV is associated with GLUT2 in liver and pancreatic β cells.

2-Deoxy-D-glucose (2DG) was first developed to inhibit glucose utilization by cancer cells (12). HKs phosphorylate 2DG to 2DG-6-phosphate, which inhibits phosphorylation of glucose. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG (http://www.ncbi.nlm.nih.gov/books/NBK23335/)) was later developed for molecular imaging studies (13). FDG is moved into cells by glucose transporters, where it is phosphorylated by HK to FDG-6-phosphate. FDG-6-phosphate cannot be metabolized further in the glycolytic pathway and remains in the cells. Tumor cells do not contain a sufficient amount of glucose-6-phosphatase to reverse the phosphorylation. The elevated rates of glycolysis and glucose transport in many types of tumor cells and activated cells enhance the uptake of FDG in these cells relative to other normal cells. Positron emission tomography (PET) with [^18^F]FDG has been used to assess alterations in glucose metabolism in brain, cancer, cardiovascular diseases, Alzheimer’s disease and other central nervous system disorders, and infectious, autoimmune, and inflammatory diseases (14-19). Various NIR dyes (such as cypate, Cy5.5, and IRDye800CW) were conjugated to 2DG (20-22) as optical imaging agents for in vivo imaging of glucose utilization in tumors in mice. Cypate is a reactive carbocyanine dye, which is derived from indocyanine green (ICG) (23). Cypate exhibits an absorbance maximum at 778 nm and an emission maximum at 805 nm, with a high extinction coefficient of 224,000 M−^1^cm−^1^. Cypate is a lipophilic dye and contains two carboxyl functional groups for covalent conjugation to the amino group of biomolecules. Guo et al. (24) evaluated cypate-2DG for in vivo NIR optical imaging in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (Hexokinase (http://www.ncbi.nlm.nih.gov/books?term=(hexokinase%20OR%20hexokinases)%20AND%20micad%5Bbook%5D), glucose transporter (http://www.ncbi.nlm.nih.gov/books?term=glucose%20transporters%20%20AND%20micad%5Bbook%5D), ICG (http://www.ncbi.nlm.nih.gov/books?term=ICG%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), Cypate (http://www.ncbi.nlm.nih.gov/books?term=Cypate%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Hexokinase (http://www.ncbi.nlm.nih.gov/gene?term=hexokinase%20human), GLUT1 (http://www.ncbi.nlm.nih.gov/gene/6513))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hexokinase (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hexokinase%5BAll+Fields%5D), GLUT1 (http://www.ncbi.nlm.nih.gov/omim/138140))
- Clinical trials ([^18^F]FDG (http://www.clinicaltrials.gov/ct2/results?term=FDG))
- Drug information in FDA ([^18^F]FDG (http://google2.fda.gov/search?q=%5B18F%5DFDG&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=9))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cypate-2DG+synthesis)]

Cypate-N-hydroxysuccinimide ester (0.0128 mmol) was reacted with 2-amino-2-DG (0.064 mmol) for 18 h at room temperature in sodium phosphate buffer (pH 9) (24). Cypate-2DG was purified with high-performance liquid chromatography and verified with mass spectroscopy. There were two 2DG molecules per cypate-2DG. The yield of cypate-2DG was ~35%, with 90% purity. Cypate-2DG displayed similar spectral properties as cypate, with maximum absorption at 782 nm and maximum emission at 821 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cypate-2DG+in+vitro)]

In vitro uptake studies of rhodamine-2DG (RhB-2DG) were performed with MCF-7/estradiol, MDA-MB-435, U87MG, and MCF-7 tumor cells in culture (24). These studies showed that high, medium, and low fluorescence intensity values correlated with the tumors' GLUT1 expression levels, respectively. Fluorescence microscopy showed that RhB-2DG accumulated in the cytoplasm of the tumor cells. Excess 2DG was able to block the NIR fluorescence signal in the cytoplasm.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cypate-2DG+rodentia)]

Guo et al. (24) performed in vivo NIR fluorescence imaging studies in nude mice (n = 5) bearing GLUT1-expressing MCF-7/estradiol xenografts at 0.5–48 h after intravenous injection of cypate-2DG (10 nmol per mouse). Cypate-2DG accumulated mainly in the tumors, with a peak tumor/muscle ratio of 14.49 ± 0.28 at 24 h; the tumor/muscle ratio gradually decreased to ~13 at 48 h. The kidney and liver exhibited strong and moderate fluorescence signals, respectively. Cypate-2DG is excreted mainly by the renal pathway and partially by the hepatobiliary pathway. Ex vivo NIR fluorescence imaging showed that the tumors exhibited the highest fluorescence intensity (tissue/muscle ratio, ~22), followed by the kidney (~13), liver (~9), lung (~8), intestine (~7), spleen (~4), and heart (~3). No blocking experiment was performed.

In the next series of experiments, NIR fluorescence imaging studies were performed in nude mice (n = 5) bearing GLUT1-expressing U87MG xenografts at 0.5–48 h after intravenous injection of cypate-2DG or cypate (10 nmol per mouse). Cypate-2DG accumulated mainly in the tumors, with a peak tumor/muscle ratio of 9 at 24 h; the tumor/muscle ratio gradually decreased to 6 at 48 h. The kidneys and liver exhibited strong and moderate fluorescence signals, respectively. On the other hand, little accumulation of cypate was observed in the tumors. The liver and kidneys exhibited strong and moderate fluorescence signals, respectively. The studies of cypate-2DG in different tumors with different expression of GLUT1 showed good correlation of tumor fluorescence intensities and GLUT1 expression levels (P < 0.05–0.001). No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cypate-2DG+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cypate-2DG+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cypate-2DG+human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Yannuzzi, L.A., Indocyanine green angiography: a perspective on use in the clinical setting. Am J Ophthalmol, 2011151(5): p. 745-751 e1.
6 Yamamoto M., Sasaguri S., Sato T. (2011). Assessing intraoperative blood flow in cardiovascular surgery. Surg Today.
7 Schaafsma B.E., Mieog J.S., Hutteman M., van der Vorst J.R., Kuppen P.J., Lowik C.W., Frangioni J.V., van de Velde C.J., Vahrmeijer A.L. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
8 Manizate F., Hiotis S.P., Labow D., Roayaie S., Schwartz M. (2010). Liver functional reserve estimation: state of the art and relevance for local treatments: the Western perspective. J Hepatobiliary Pancreat Sci.
9 Smith T.A. (2000). Mammalian hexokinases and their abnormal expression in cancer. Br J Biomed Sci.
10 Suolinna E.M., Haaparanta M., Paul R., Harkonen P., Solin O., Sipila H. (1986). Metabolism of 2-[18F]fluoro-2-deoxyglucose in tumor-bearing rats: chromatographic and enzymatic studies. Int J Rad Appl Instrum B.
11 Wood I.S., Trayhurn P. (2003). Glucose transporters (GLUT and SGLT): expanded families of sugar transport proteins. Br J Nutr.
12 Laszlo J., Humphreys S.R., Goldin A. (1960). Effects of glucose analogues (2-deoxy-D-glucose, 2-deoxy-D-galactose) on experimental tumors. J Natl Cancer Inst.
13 Fowler J.S., Ido T. (2002). Initial and subsequent approach for the synthesis of 18FDG. Semin Nucl Med.
14 Phelps M.E. (2000). PET: the merging of biology and imaging into molecular imaging. J Nucl Med.
15 Phelps M.E., Mazziotta J.C. (1985). Positron emission tomography: human brain function and biochemistry. Science.
16 Phelps M.E., Mazziotta J.C., Huang S.C. (1982). Study of cerebral function with positron computed tomography. J Cereb Blood Flow Metab.
17 Rohren E.M., Turkington T.G., Coleman R.E. (2004). Clinical applications of PET in oncology. Radiology.
18 Sokoloff L. (1985). Basic principles in imaging of regional cerebral metabolic rates. Res Publ Assoc Res Nerv Ment Dis.
19 Spence A.M., Mankoff D.A., Muzi M. (2003). Positron emission tomography imaging of brain tumors. Neuroimaging Clin N Am.
20 Kovar J.L., Volcheck W., Sevick-Muraca E., Simpson M.A., Olive D.M. (2009). Characterization and performance of a near-infrared 2-deoxyglucose optical imaging agent for mouse cancer models. Anal Biochem.
21 Cheng Z., Levi J., Xiong Z., Gheysens O., Keren S., Chen X., Gambhir S.S. (2006). Near-infrared fluorescent deoxyglucose analogue for tumor optical imaging in cell culture and living mice. Bioconjug Chem.
22 Chen Y., Zheng G., Zhang Z.H., Blessington D., Zhang M., Li H., Liu Q., Zhou L., Intes X., Achilefu S., Chance B. (2003). Metabolism-enhanced tumor localization by fluorescence imaging: in vivo animal studies. Opt Lett.
23 Ye Y., Bloch S., Kao J., Achilefu S. (2005). Multivalent carbocyanine molecular probes: synthesis and applications. Bioconjug Chem.
24 Guo J., Du C., Shan L., Zhu H., Xue B., Qian Z., Achilefu S., Gu Y. (2012). Comparison of near-infrared fluorescent deoxyglucose probes with different dyes for tumor diagnosis in vivo. Contrast Media Mol Imaging.